# ^111^In-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetracetic acid-Glu{PEG_4_-Glu[cyclo(Lys-Arg-Gly-Asp-D-Phe)]-cyclo(Lys-Arg-Gly-Asp-D-Phe)}-{PEG_4_-Glu[cyclo(Lys-Arg-Gly-Asp-D-Phe)]-cyclo(Lys-Arg-Gly-Asp-D-Phe)} (PEG_4_ = 15 amino-4,710,13-tetraoxapentadecanoic acid)

Chemical name: | ^111^In-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetracetic acid-Glu{PEG_4_-Glu[cyclo(Lys-Arg-Gly-Asp-D-Phe)]-cyclo(Lys-Arg-Gly-Asp-D-Phe)}-{PEG_4_-Glu[cyclo(Lys-Arg-Gly-Asp-D-Phe)]-cyclo(Lys-Arg-Gly-Asp-D-Phe)} (PEG_4_ = 15 amino-4,710,13-tetraoxapentadecanoic acid) | [image]
Abbreviated name: | ^111^In(DOTA-2P-RGD_4_) | [image]
Synonym: | ^111^In-DOTA-E{PEG_4_-E[c(RGDfK)]_2_}_2_ | [image]
Agent Category: | Peptides | [image]
Target: | Integrin alphavbeta3 (α_v_β_3_) | [image]
Target Category: | Receptors | [image]
Method of detection: | Single-photon emission computed tomography (SPECT) or planar imaging | [image]
Source of signal / contrast: | ^111^In | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structures of ^111^In(DOTA-2P-RGD_4_) by Shi et al. (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Integrin%20%u03B1v%u03B23%20and%20imaging)]

The ^111^In-labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetracetic acid (DOTA)-Glu{PEG_4_-Glu[cyclo(Lys-Arg-Gly-Asp-D-Phe)]-cyclo(Lys-Arg-Gly-Asp-D-Phe)}-{PEG_4_-Glu[cyclo(Lys-Arg-Gly-Asp-D-Phe)]-cyclo(Lys-Arg-Gly-Asp-D-Phe)} (PEG_4_ = 15 amino-4,710,13-tetraoxapentadecanoic acid), abbreviated as ^111^In(DOTA-2P-RGD_4_) or ^111^In-DOTA-E{PEG_4_-E[c(RGDfK)]_2_}_2_, was synthesized by Shi et al. as an agent for molecular imaging of tumor angiogenesis by targeting integrin alphavbeta3 (α_v_β_3_) (1). Here, P = PEG_4_ = 15 amino-4,710,13-tetraoxapentadecanoic acid = a linker between two c(RGDfK) motifs; c(RGDfK) = cyclo(Lys-Arg-Gly-Asp-D-Phe); RGD_4_ = four motifs of c(RGDfK); and E = Glu.

Integrin α_v_β_3_ is a receptor that is overexpressed on the activated endothelial cells of tumors (2). Because the integrin α_v_β_3_ binds with extracellular matrix proteins (e.g., vitronectin, fibronectin) through the exposed Arg-Gly-Asp tripeptide sequence, RGD-containing peptides have been intensively studied in the past decade as a vector for imaging α_v_β_3_ expression (3, 4). Although significant progress has been made, improving the binding affinity and pharmacokinetics of RGD peptides remains the major consideration in the design of agents, and various strategies have been developed for this improvement, such as the use of RGD multimers, the introduction of sugar amino acids or D-amino acids into the RGD peptides, and the conjugation of the RGD peptides with chelators or polyethylene glycol (PEG) chains (5, 6).

The concept of multimerization has been developed to address the question of multimeric binding by "poly-potent" ligands. Multimers are formed by bridging monomeric units through linker(s) (2, 7). The multimer effect has been demonstrated in different studies, showing that the binding affinity of RGD peptides increases in the order of monomer < dimer < tetramer < octamer. For example, the cyclo(-RGDfE-)-monomer, dimer, and tetramer containing heptaethylene glycol spacer units have been shown to exhibit α_v_β_3_-binding affinities that increase by a factor of ten with each duplication of binding units (8). The integrin affinity of the DOTA-RGD octamer has been shown to be three-fold higher than that of the DOTA-RGD tetramer (7).

Recently, investigators from Purdue University suggested a concept of "bivalency" for the α_v_β_3_-binding affinity of RGD-containing peptides (1, 6, 9). The main point of this concept is that the multimeric cyclic RGD peptides are likely bivalent rather than multivalent in binding to integrin α_v_β_3_, and enough distance between two RGD motifs is the key for bivalency (1, 5, 10). For example, the dimeric peptide E[c(RGDfK)]_2_ (RGD_2_) is monovalent, whereas the dimeric peptides PEG_4_-E[PEG_4_-c(RGDfK)]_2_ (3P-RGD_2_) and G_3_-E[G_3_-c(RGDfK)]_2_ (3G-RGD_2_) (G = G_3_ = Gly-Gly-Gly linker) are bivalent because of the increased distance between the two cyclic RGD motifs for simultaneous integrin α_v_β_3_ binding in the latter two peptides (5). The cyclic RGD tetramers, such as DOTA-RGD_4_ and DOTA-E{G_3_-E[G_3_-c(RGDfK)]_2_}_2_ (DOTA-6G-RGD_4_), are also likely bivalent in binding to integrin α_v_β_3_ even though they contain four identical RGD motifs (5, 10). Studies with three other tetramers (DOTA-2P-RGD_4_, DOTA-2P4G-RGD_4_, and DOTA-6P-RGD_4_) have further shown that the three tetramers are not tetravalent, although the tetramers exhibited a higher binding affinity to α_v_β_3_ than monomers and dimers, and the "locally enriched" RGD concentration has been considered to contribute to the higher binding affinity (1, 6). The linkers between RGD motifs may have a significant impact on the integrin α_v_β_3_-targeting capability, biodistribution, excretion kinetics, and metabolic stability of cyclic RGD peptides (1, 11, 12).

This chapter summarizes the data obtained with ^111^In(DOTA-2P-RGD_4_). Other chapters summarize the data obtained with ^111^In(DOTA-6P-RGD_4_) and ^111^In(DOTA-2P4G-RGD_4_), respectively.

### Related Resource Links:

The nucleotide (http://www.ncbi.nlm.nih.gov/nuccore?term=integrin%20%CE%B1v%CE%B23) and protein (http://www.ncbi.nlm.nih.gov/protein?term=integrin%20%CE%B1v%CE%B23) sequences of integrin α_v_β_3_

Integrin α_v_β_3_-related imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=integrin+%CE%B1v%CE%B23+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Articles of integrin α_v_β_3_ (http://www.ncbi.nlm.nih.gov/omim?term=integrin%20%CE%B1v%CE%B23) in Online Mendelian Inheritance in Man

Integrin α_v_β_3_-related clinical trials (http://clinicaltrials.gov/ct2/results?term=integrin+%CE%B1v%CE%B23) in ClinicTrial.gov

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%2021850213)]

The RGD-containing peptides were all custom-made, including P-RGD, P2G-RGD_2_, 3P-RGD_2_, and 3P-RGK_2_ (RGK = cyclo(Arg-Gly-Lys-D-Phe-Asp)). The tetramers were synthesized by the reaction of Boc-E(OSu)_2_ and their corresponding dimers (1). Conjugation of the RGD peptides with DOTA-OSu resulted in their corresponding conjugates (DOTA-P-RGD, DOTA-P-RGD_2_, DOTA-3P-RGD_2_, DOTA-2P-RGD_4_, DOTA-2P4G-RGD_4_, and DOTA-6P-RGD_4_, respectively). DOTA-6P-RGK_4_ was prepared using a procedure identical to that for DOTA-6P-RGD_4_. DOTA-6P-RGK_4_ has the identical amino acids, but its sequence is scrambled to demonstrate the RGD-specificity of DOTA-6P-RGD_4_. The identities for all RGD conjugates were confirmed, and their purities were all >95% before being used for ^111^In labeling and determination of their integrin α_v_β_3_ binding affinity. Table 1 lists the molecular weights and yields of each DOTA-conjugated peptide (1).

Table 1: The physicochemical characteristics of the RGD peptides.

Agents | DOTA-P-RGD | DOTA-P-RGD_2_ | DOTA-3P-RGD_2_* | DOTA-2P-RGD_4_ | DOTA-2P4G-RGD_4_ | DOTA-6P-RGD_4_ | DOTA-6P-RGK_4_
MW | 1,237.58 | 1,951.5 | 2,447.35 | 3,626.4 | 4,315.4 | 4,622.7 | 4,622.7
Yield | ~40% | ~41% | ~30% | ~56% | ~64% | ~43% | ~68%

*The data for DOTA-3P-RGD_2_ were obtained from Shi et al. (5).

All ^111^In-labeled peptides were prepared by reacting ^111^InCl_3_ with the respective DOTA conjugates in NH_4_OAc buffer (100 mM, pH = 5.5). Radiolabeling was completed by heating the reaction mixture at 100°C for ~15 min. After purification, the radiochemical purity was >95% and the specific activity was >40 mCi/μmol (1.48 GBq/µmol) for all ^111^In-labeled RGD peptides (1).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%2021850213)]

The integrin binding affinity and specificity of the RGD peptides were assessed in U87MG human glioma whole cells, with ^125^I-c(RGDyK) as the integrin-specific radioligand (1). The α_v_β_3_ binding affinity of the peptides followed the order of DOTA-6P-RGD_4_ ~ DOTA-2P4G-RGD_4_ ~ DOTA-2P-RGD_4_ > DOTA-P-RGD_2_ > DOTA-P-RGD > RGD (IC_50_ = 49.9) (Table 1). The binding affinity of DOTA-3P-RGD_2_ was significantly higher than that of DOTA-P-RGD and DOTA-P-RGD_2_ (P < 0.01). However, the investigators found that the integrin α_v_β_3_ binding affinities of DOTA-2P-RGD_4_, DOTA-2P4G-RGD_4_, and DOTA-6P-RGD_4_ were only marginally higher than that of DOTA-3P-RGD_2_, suggesting that they might share the same bivalency in binding to the integrin α_v_β_3_.

Shi et al. also determined the water-octanol partition coefficients and stability of the ^111^In-labeled peptides (1). The log P values are listed in Table 2. The ^111^In-labeled peptides remained stable for >72 h after purification in the presence of 3 mM EDTA.

Table 2: The IC_50_ and log P values of the ^111^In-labeled cyclic RGD peptides.

Peptides | DOTA-P-RGD | DOTA-P-RGD_2_ | DOTA-3P-RGD_2_ | DOTA-2P-RGD_4_ | DOTA-2P4G-RGD_4_ | DOTA-6P-RGD_4_ | DOTA-6P-RGK_4_
IC_50_ (nM) | 44.3 | 5.0 | 1.5 | 0.5 | 0.2 | 0.3 | 437
Log P | -3.48 | -3.22 | -4.20 | -3.87 | -3.93 | -3.68 | -3.61

IC_50_: half-maximal inhibitory concentration.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%2021850213)]

Biodistribution, imaging, and metabolic studies were performed in athymic nude mice bearing U87MG human glioma xenografts in both left and right upper flanks (1).

For the biodistribution studies, each mouse was administered ~3 μCi (~0.111 MBq) of the agent via tail vein injection (1). Mice were then euthanized at 0.5, 1, 4, 24, and 72 h after injection (n = 5 mice/time point). The organ uptake was calculated as the percentage of injected dose per gram of organ mass (% ID/g). The tumor and intestinal uptake values of ^111^In(DOTA-2P-RGD_4_) were high and close to those of ^111^In(DOTA-6P-RGD_4_) over the 72-h period. ^111^In(DOTA-2P-RGD_4_) also had a rapid clearance from normal organs, such as the blood, kidneys, and liver. Therefore, the tumor/liver and tumor/kidney ratios for ^111^In(DOTA-2P-RGD_4_) were comparable to those obtained for ^111^In(DOTA-6P-RGD_4_) and ^111^In(DOTA-6G-RGD_4_.

Table 3: Selected biodistribution data of ^111^In(DOTA-2P-RGD_4_).

% ID/g | 0.5 h | 1 h | 24 h | 72 h
Blood | 1.12 ± 0.08 | 0.31 ± 0.16 | 0.03 ± 0.00 | 0.02 ± 0.02
U87MG | 12.98 ± 5.99 | 10.66 ± 2.4 | 6.52 ± 3.85 | 2.87 ± 1.45
Tumor/Blood | 11.60 ± 5.36 | 34.67 ± 7.84 | 231.33 ± 136.67 | 192.06 ± 172.1
Tumor/Kidney | 1.46 ± 0.67 | 1.60 ± 0.27 | 1.46 ± 0.80 | 1.28 ± 0.59
Tumor/Liver | 6.09 ± 2.81 | 4.34 ± 1.12 | 4.19 ± 1.04 | 4.89 ± 1.62
Tumor/Lungs | 4.06 ± 1.88 | 4.31 ± 0.96 | 6.76 ± 3.99 | 8.94 ± 5.37
Tumor/Muscle | 13.92 ± 6.43 | 11.76 ± 3.58 | 16.78 ± 9.92 | 25.87 ± 15.57

No blocking experiment was performed with ^111^In(DOTA-2P-RGD_4_). The blocking experimental data obtained with ^111^In(DOTA-6P-RGD_4_) are summarized in the chapter on ^111^In(DOTA-6P-RGD_4_) in MICAD (1).

The imaging studies were performed after tail vein administration of ~100 μCi (3.7 MBq) ^111^In(DOTA-2P-RGD_4_) (n = 3 mice) (1). The whole-body images were acquired at 0.5, 1, 4, 24, and 72 h after injection. The tumors were clearly visualized with excellent tumor/background contrast as early as 1 h after injection. A long tumor retention time was observed, which was consistent with the biodistribution results. The time to half-maximal radioactivity in tumors was >30 h for ^111^In(DOTA-2P-RGD_4_), ^111^In(DOTA-2P4G-RGD_4_), and ^111^In(DOTA-6P-RGD_4_) (1).

For the metabolism studies, each mouse was given ~100 μCi (3.7 MBq) ^111^In(DOTA-6P-RGD_4_) via tail vein injection (1). The urine samples were collected at 30 min and 120 min after injection, and the feces samples were collected at 120 min. The percentage of radioactivity recovery was >95% (by γ-counting) for both urine and feces. There were very limited radioactivity accumulation in the liver and kidneys. There was little metabolism detected in the urine or feces samples over the 2-h study period for ^111^In(DOTA-2P-RGD_4_).

Shi et al. comparatively analyzed the biodistribution data for ^111^In(DOTA-2P-RGD_4_), ^111^In(DOTA-2P4G-RGD_4_), ^111^In(DOTA-6P-RGD_4_), ^111^In(DOTA-6G-RGD_4_), ^111^In(DOTA-3P-RGD_2_), ^111^In(DOTA-P-RGD_2_), and ^111^In(DOTA-P-RGD) (1). Over the first 24 h, the tumor uptake difference between the tetramers and dimers was not significant (P > 0.05). The tumor uptake at 72 h (% ID/g) followed the general order of ^111^In(DOTA-6P-RGD_4_) (3.04) > ^111^In(DOTA-2P-RGD_4_) (2.87) ~ ^111^In(DOTA-2P4G-RGD_4_) (2.66) > ^111^In(DOTA-3P-RGD_2_) (2.18), which was similar to the trend observed with integrin α_v_β_3_ binding affinity (IC_50_, nM) of DOTA-6P-RGD_4_ (0.3 ± 0.1) ~ DOTA-2P4G-RGD_4_ (0.2 ± 0.1) ~ DOTA-2P-RGD_4_ (0.5 ± 0.1) > DOTA-3P-RGD_2_ (1.5 ± 0.2). Among the ^111^In-labeled radiotracers, ^111^In(DOTA-6G-RGD_4_) had the highest uptake in the tumor and intestine at 72 h after injection. The half-life of ^111^In(DOTA-6G-RGD_4_) in the tumor was estimated to be 60 h. In contrast, ^111^In(DOTA-3P-RGD_2_) and ^111^In(DOTA-2P4G-RGD_4_) had low uptake in the intestine, kidneys, and liver over the 72-h period. As a result, ^111^In(DOTA-3P-RGD_2_) and ^111^In(DOTA-2P4G-RGD_4_) had tumor/kidney and tumor/liver ratios that were significantly better (P < 0.05) than those of ^111^In(DOTA-6G-RGD_4_) and ^111^In(DOTA-6P-RGD_4_) during that period of time. As expected, ^111^In(DOTA-P-RGD) had the lowest tumor uptake (3.7% ID/g and 0.7% ID/g at 0.5 h and 72 h after injection, respectively). ^111^In(DOTA-P-RGD_2_) had a relatively high tumor uptake (6.1 at 0.5 h after injection), but it had a significant washout from the tumor, with uptake values being 4.9, 4.8, 3.1 and 1.6% ID/g at 1, 4, 24, and 72 h after injection, respectively. The tumor uptake values follow the trend of ^111^In(DOTA-3P-RGD_2_) > ^111^In(DOTA-P-RGD_2_) > ^111^In(DOTA-P-RGD), which was consistent with the order of their α_v_β_3_ binding affinities (IC_50_ value): DOTA-3P-RGD_2_ < DOTA-P-RGD_2_ < DOTA-P-RGD.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term)]

No references are currently available.

## References

1 Shi J., et al. (2011). Evaluation of In-Labeled Cyclic RGD Peptides: Effects of Peptide and Linker Multiplicity on Their Tumor Uptake, Excretion Kinetics and Metabolic Stability. Theranostics.
2 Dijkgraaf I., Beer A.J., Wester H.J. (2009). Application of RGD-containing peptides as imaging probes for alphavbeta3 expression. Front Biosci.
3 Gaertner, F.C., M. Schwaiger, and A.J. Beer, Molecular imaging of avb3 expression in cancer patients. Q J Nucl Med Mol Imaging, 2010
4 Lu, X. and R.F. Wang, A Concise Review of Current Radiopharmaceuticals in Tumor Angiogenesis Imaging. Curr Pharm Des, 2012
5 Shi J., et al. (2011). Impact of bifunctional chelators on biological properties of 111In-labeled cyclic peptide RGD dimers. Amino Acids.
6 Liu S. (2009). Radiolabeled cyclic RGD peptides as integrin alpha(v)beta(3)-targeted radiotracers: maximizing binding affinity via bivalency. Bioconjug Chem.
7 Li Z.B., et al. (2007). (64)Cu-labeled tetrameric and octameric RGD peptides for small-animal PET of tumor alpha(v)beta(3) integrin expression. J Nucl Med.
8 Poethko T., et al. (2004). Chemoselective pre-conjugate radiohalogenation of unpretected mono- and multimeric peptides via oxime formation. Radiochim Acta.
9 Chakraborty S., et al. (2010). Evaluation of 111In-labeled cyclic RGD peptides: tetrameric not tetravalent. Bioconjug Chem.
10 Shi J., et al. (2009). Improving tumor uptake and pharmacokinetics of (64)Cu-labeled cyclic RGD peptide dimers with Gly(3) and PEG(4) linkers. Bioconjug Chem.
11 Liu Z., et al. (2009). (68)Ga-labeled cyclic RGD dimers with Gly3 and PEG4 linkers: promising agents for tumor integrin alphavbeta3 PET imaging. Eur J Nucl Med Mol Imaging.
12 Shi J., et al. (2008). Improving tumor uptake and excretion kinetics of 99mTc-labeled cyclic arginine-glycine-aspartic (RGD) dimers with triglycine linkers. J Med Chem.